# Gold-polyethylene glycol nanoshells

Chemical name: | Gold-polyethylene glycol nanoshells
Abbreviated name: | Au-PEG-nanoshells
Synonym:
Agent Category: | Metal
Target: | Phagocytes and tumor cells
Target Category: | Phagocytosis, passive targeting
Method of detection: | Optical coherence tomography (OCT)
Source of signal: | Au
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gold+nanoshells)]

Optical fluorescence imaging is increasingly used to visualize biological functions of specific targets (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in small animals.

Optical tunable nanoshells are nanocrystals made of an insulating core and a metal outer shell (3). They can be tuned in a range of wavelengths for NIR absorption, thus providing broad excitation profiles and high absorption coefficients. They can be coated and capped with hydrophilic materials for additional conjugation with biomolecules, such as peptides, antibodies, nucleic acids, and small organic compounds for in vitro and in vivo studies (4-7). Gold nanoshells have a silica core (~110 nm in diameter) and a gold shell (~10 nm thick) (8). The gold nanoshells are coated with polyethylene glycol (Au-PEG-nanoshells) to reduce aggregation of nanoshells and protein absorption in blood (9). These nanoshells had a peak absorption resonance of 800–830 nm. Gold nanoshells are being studied as cancer imaging and photothermal agents.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gold+nanoshells+synthesis)]

Gobin et al. (8) produced gold nanoshells using methods previously reported (10). Organosilane molecules (3-aminopropyltriethoxysilane) were adsorbed onto silica nanoparticles as dielectric cores. These molecules bond to the surface of the silica nanoparticles, extending their amine groups outward as a new termination of the nanoparticle surface. The isolated silane-coated silica nanoparticles were added to a solution of gold nanoparticles (2–4 nm in diameter). The gold particles bond covalently to the organosilane linkage molecules via the amine group. The nanoshells were then treated with chloroauric acid to form a contiguous gold shell. The nanoshells had cores 119 ± 11 nm in diameter and gold shells ~12 nm thick. The shells were coated with PEG (5 kDa) to stabilize them and to reduce aggregation of nanoshells and protein absorption in blood. These nanoshells have a peak absorption resonance of 800–830 nm. The nanoshell gold content is estimated to be 8.76 × 10^-15^ g/Au-PEG-nanoshell.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gold+nanoshells+in+vitro)]

Hirsch et al. (9) performed phase contrast microscopy using human breast epithelial carcinoma SK-BR-3 cells after incubation with Au-PEG-nanoshells at 37°C for 1 h in protein-free medium. Silver staining of the treated cells after washing showed high densities of nanoshells bound to the cells. No silver staining was observed with the buffer-treated cells. Only the nanoshell-treated cells were photothermally destroyed by laser exposure at 35 W/cm^2^ for 7 min.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gold+nanoshells+%20rodentia)]

James et al. (11) studied long-term biodistribution in normal mice up to 28 days after intravenous injection of 2.4 × 10^10^ Au-PEG-nanoshells/mouse. Gold concentrations in blood and excised tissues were measured with neutron activation analysis. Au-PEG-nanoshells accumulated quickly in macrophages in the liver and spleen. Au-PEG-nanoshells had a half-life of 3.7 h in blood. Au-PEG-nanoshells were not detected in the blood at 48 h. The tissue with the highest gold accumulation at 7 days was the spleen (2.8 mg/g), followed by the liver (0.31 mg/g), kidney (0.021 mg/g), and lung (0.006 mg/g). Little accumulation was observed in the muscle, brain, and bone. Elevated levels of gold were still present in the liver and spleen at 28 days, whereas some clearance by the kidney and lung was observed. No physiological complications were observed in the mice at 28 days. In mice bearing subcutaneous mouse colon carcinoma CT-26 tumors (~0.5 cm in diameter), gold levels in various excised tissues were measured at 1, 4, 24, and 48 h after injection of Au-PEG-nanoshells. Gold concentration in the tumor was 20 parts per million (ppm) at 1 h, 62 ppm at 4 h, 102 ppm at 24 h, and 62 ppm at 48 h. In contrast, the gold concentration in the lung was 68 ppm at 1 h, 45 ppm at 4 h, 18 ppm at 24 h, and 4 ppm at 48 h. The ratio of tumor accumulation to accumulation in the brain, muscle, bone, blood, lung, kidney, and spleen at 24 h was 188, 20, 17, 8, 7, 3, and 0.06, respectively.

Gobin et al. (8) performed optical coherence tomography imaging in mice bearing subcutaneous mouse colon carcinoma CT-26 tumors at 20 h after intravenous injection of Au-PEG-nanoshells or saline (control). There was a 56% increase in optical coherence tomography image brightness of tumor over the muscle (P < 0.00002), whereas little enhancement was observed in the mice injected with saline. The presence of Au-PEG-nanoshells was confirmed with silver staining of the tumor tissue from mice injected with nanoshells. Thus, the leakiness of the tumor allows accumulation of Au-PEG-nanoshells within the tumor by passive diffusion.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gold+nanoshells+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gold+nanoshells+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gold+nanoshells+human)]

No publication is currently available.

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Hirsch L.R., Gobin A.M., Lowery A.R., Tam F., Drezek R.A., Halas N.J., West J.L. (2006). Metal nanoshells. Ann Biomed Eng.
4 Bernardi R.J., Lowery A.R., Thompson P.A., Blaney S.M., West J.L. (2008). Immunonanoshells for targeted photothermal ablation in medulloblastoma and glioma: an in vitro evaluation using human cell lines. J Neurooncol.
5 Hauck T.S., Chan W.C. (2007). Gold nanoshells in cancer imaging and therapy: towards clinical application. Nanomed.
6 Stern J.M., Stanfield J., Kabbani W., Hsieh J.T., Cadeddu J.A. (2008). Selective prostate cancer thermal ablation with laser activated gold nanoshells. J Urol.
7 Zahr A.S., Pishko M.V. (2007). Encapsulation of paclitaxel in macromolecular nanoshells. Biomacromolecules.
8 Gobin A.M., Lee M.H., Halas N.J., James W.D., Drezek R.A., West J.L. (2007). Near-infrared resonant nanoshells for combined optical imaging and photothermal cancer therapy. Nano Lett.
9 Hirsch L.R., Stafford R.J., Bankson J.A., Sershen S.R., Rivera B., Price R.E., Hazle J.D., Halas N.J., West J.L. (2003). Nanoshell-mediated near-infrared thermal therapy of tumors under magnetic resonance guidance. Proc Natl Acad Sci U S A.
10 Oldenburg S.J., Averitt R.D., Westcott S.L., Halas N.J. (1998). Nanoengineering of optical resonances. Chemical Physics Letters.
11 James W.D., Hirsch L.R., West J.L., O'Neal P.D., Payne J.D. (2007). Application of INAA to the build-up and clearance of gold nanoshells in clinical studies in mice. Journal of Radioanalytical and Nuclear Chemistry.